# L-Methyl-methionine-indocyanine green derivative 02

Chemical name: | L-Methyl-methionine-indocyanine green derivative 02
Abbreviated name: | Met-ICG-Der-02
Synonym: | ICG-Der-02-Met
Agent category: | Compound
Target: | L-type amino acid transporter 1/2 (LAT1/2)
Target category: | Transporter
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | ICG-Der-02
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Met-ICG-Der-02)]

A variety of ^11^C- and ^18^F-labeled amino acids have been studied for potential use in positron emission tomography (PET) oncology (1, 2). Most brain tumors show an increased uptake of amino acids as compared with normal brain tissues (3). These amino acids are composed of naturally occurring amino acids, such as L-[^11^C]leucine, S-[^11^C]methyl-L-methionine ([^11^C]MET), and L-[^11^C]tyrosine, and non-natural amino acids, such as [^11^C]aminoisobutyric acid, [^11^C]1-aminocyclopentane-1-carboxylic acid, and [^11^C]1-aminocyclobutane-1-carboxylic acid. ^123^I-Labeled amino acids are also used in oncological imaging (1, 4, 5). Some 20 amino acid transporter systems have been identified (1). Most amino acids are taken up by tumor cells through an energy-independent L-type amino acid transporter system, a Na-dependent transporter system A, or a Na^+^-dependent system B^0^ (6). They are retained in tumor cells due to their metabolic activities, including incorporation into proteins, which are higher than most normal cells (1). Malignant transformation increases the use of amino acids for energy, protein synthesis, and cell division. Tumor cells have been found to have overexpressed transporter systems (7). L-[^11^C]MET, [^18^F]fluorotyrosine, L-[^11^C]leucine, and [^18^F]fluoro-α-methyl tyrosine have been widely used in the detection of tumors (2, 6) but are not approved by the United States Food and Drug Administration. These agents are moved into cells by various amino acid transporters and are incorporated into proteins. The fraction of radiolabeled amino acid that is incorporated into protein is usually small compared to the total amount taken up into the cell, except for leucine, which is quantitatively incorporated into proteins. These natural amino acid imaging agents are based on amino acid transport and protein incorporation.

[^11^C]MET has been widely used in the detection of brain, head and neck, lung, and breast cancers, as well as lymphomas (2) [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20and%20methionine%20and%20human%20and%20neoplasm)]. [^11^C]MET can cross the blood–brain barrier, and while it is incorporated mainly into proteins, [^11^C]MET is also incorporated into lipid, RNA, and DNA. [^11^C]MET PET imaging is more sensitive to radiotherapy compared to [^18^F]FDG and is useful for monitoring treatment of cancer. Among the various optical imaging agents, only indocyanine green (ICG (http://dailymed.nlm.nih.gov/dailymed/drugInfo.cfm?id=15096)), with NIR fluorescence absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment (8-11). It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications, such as optical imaging and mapping of both the lymphatic vessels and lymph nodes in cancer patients for surgical dissection of tumor cells, as well as endoscopic imaging of the pancreas and colon. ICG derivative 02 (ICG-Der-02) contains one carboxyl functional group for covalent conjugation to the amino group of biomolecules. ICG-Der-02 is a hydrophilic dye. Mahounga et al. (12) evaluated Met-ICG-Der-02 for in vivo NIR optical imaging in tumor-bearing mice.

### Related Resource Links:

- Chapters in MICAD (amino acid transporters (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=amino%20acid%20(transporter%20OR%20transporters)+AND+micad%5Bbook%5D), methionine (http://www.ncbi.nlm.nih.gov/books?term=methionine%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D), ICG (http://www.ncbi.nlm.nih.gov/books?term=ICG%5BAll%20Fields%5D%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (L-type amino acid transporter 1 (http://www.ncbi.nlm.nih.gov/gene/8140), L-type amino acid transporter 2 (http://www.ncbi.nlm.nih.gov/gene/23428), A-type amino acid transporter (http://www.ncbi.nlm.nih.gov/gene/54407))
- Articles in Online Mendelian Inheritance in Man (OMIM) (amino acid transporters (http://www.ncbi.nlm.nih.gov/omim?Db=omim&Cmd=DetailsSearch&Term=amino%5BAll+Fields%5D+AND+acid%5BAll+Fields%5D+AND+transporter%5BAll+Fields%5D))
- Clinical trials (amino acid transporters (http://www.clinicaltrials.gov/ct2/results?term=amino+acid+transporters), L-[^11^C]methionine (http://www.clinicaltrials.gov/ct2/results?term=11C+MET), ICG (http://www.clinicaltrials.gov/ct2/results?term=ICG))
- Drug information in FDA (amino acid transporters (http://google2.fda.gov/search?q=amino+acid+transporters&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=13&y=15), L-[^11^C]methionine (http://google2.fda.gov/search?q=11C-methionine+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=8&y=8), ICG (http://google2.fda.gov/search?q=Indocyanine+Green&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=4&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Met-ICG-Der-02%20and%20synthesis)]

ICG-Der-02-N-hydroxysuccinimide ester (0.02 mmol) was reacted with Met (0.067 mmol) for 18 h at room temperature in Tris buffer (pH 8) (12). Met-ICG-Der-02 was purified with column chromatography and verified with mass spectroscopy. There is one Met molecule per Met-ICG-Der-02 conjugate. The yield and purity of Met-ICG-Der-02 were not reported. Met-ICG-Der-02 displayed spectral properties similar to those of ICG-Der-02, with maximum absorption at 783 nm and maximum emission at 811 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Met-ICG-Der-02%20and%20in%20vitro)]

Reverse transcriptase polymerase chain reaction showed that PC3 human prostate cancer cells and MDA-MB-231 human breast cancer cells exhibited levels of LAT1 and LAT2 five times higher than HELF normal human lung fibroblast cells (12). In vitro uptake studies of Rhodamine-Met (RhB-Met) were performed with these cells in culture showing that high fluorescence intensity in PC3 and MDA-MB-231 cells with negligible signal in HELF cells correlated well with their LAT1/2 expression levels. Excess Met or Met-ICG-Der-02 was able to completely block the fluorescence signal in MDA-MB-231. RhB was used because the investigators do not have confocal fluorescence microcopy with NIR capability.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Met-ICG-Der-02%20and%20rodentia)]

Mahounga et al. (12) performed in vivo whole-body NIR fluorescence imaging studies in normal nude mice (n = 5) at 0.5–24 h after injection of 22.5 µmol/kg Met-ICG-Der-02 or ICG-Der-02. Images showed that NIR fluorescence spread all over the body at 0.5 h and then concentrated in the liver and kidneys. Most NIR fluorescence was cleared from the body by 24 h. Ex vivo imaging of the main organs (the liver, kidney, lung, stomach, intestine, urinary bladder, heart, and spleen) of mice was performed at 0.5, 2, 5, and 12 h. NIR fluorescence was initially detected in all the organs and gradually migrated to the liver, intestine, and kidney at 5–12 h. Met-ICG-Der-02 was excreted by the liver and kidneys. ICG-Der-02 exhibited rapid clearance by 4 h after injection via the liver and kidneys in normal nude mice (n = 5). No NIR fluorescence was observed in the liver at 4 h or the intestine throughout the time course of the experiment. ICG-Der-02 was mainly excreted by the kidneys.

Mahounga et al. (12) performed in vivo whole-body NIR fluorescence imaging studies in nude mice (n = 5/group) bearing MDA-MB-231 or PC3 xenografts at 0.5–48 h after injection of 22.5 µmol/kg Met-ICG-Der-02. Both tumors were clearly visualized by 2 h after injection. The peak tumor/muscle ratios were ~7 and ~8.5 at 12 h for MDA-MB-231 and PC3 tumors, respectively. NIR fluorescence decreased gradually to background level by 48 h. Co-injection with excess Met completely blocked NIR fluorescence in the MDA-MB-231 tumors as well as other main organs, except the urinary bladder, at 4–12 h after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Met-ICG-Der-02%20and%20%28pig%20or%20dog%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Met-ICG-Der-02%20AND%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Met-ICG-Der-02%20and%20human)]

No publication is currently available.

## References

1 Jager P.L., Vaalburg W., Pruim J., de Vries E.G., Langen K.J., Piers D.A. (2001). Radiolabeled amino acids: basic aspects and clinical applications in oncology. J Nucl Med.
2 Laverman P., Boerman O.C., Corstens F.H., Oyen W.J. (2002). Fluorinated amino acids for tumour imaging with positron emission tomography. Eur J Nucl Med Mol Imaging.
3 Herholz K., Heiss W.D. (2004). Positron emission tomography in clinical neurology. Mol Imaging Biol.
4 Langen K.J., Pauleit D., Coenen H.H. (2002). 3-[(123)I]Iodo-alpha-methyl-L-tyrosine: uptake mechanisms and clinical applications. Nucl Med Biol.
5 Lahoutte T., Caveliers V., Camargo S.M., Franca R., Ramadan T., Veljkovic E., Mertens J., Bossuyt A., Verrey F. (2004). SPECT and PET amino acid tracer influx via system L (h4F2hc-hLAT1) and its transstimulation. J Nucl Med.
6 Langen K.J., Jarosch M., Muhlensiepen H., Hamacher K., Broer S., Jansen P., Zilles K., Coenen H.H. (2003). Comparison of fluorotyrosines and methionine uptake in F98 rat gliomas. Nucl Med Biol.
7 Saier M.H., Daniels G.A., Boerner P., Lin J. (1988). Neutral amino acid transport systems in animal cells: potential targets of oncogene action and regulators of cellular growth. J Membr Biol.
8 Yannuzzi, L.A., Indocyanine green angiography: a perspective on use in the clinical setting. Am J Ophthalmol, 2011151(5): p. 745-751 e1.
9 Yamamoto M., Sasaguri S., Sato T. (2011). Assessing intraoperative blood flow in cardiovascular surgery. Surg Today.
10 Schaafsma B.E., Mieog J.S., Hutteman M., van der Vorst J.R., Kuppen P.J., Lowik C.W., Frangioni J.V., van de Velde C.J., Vahrmeijer A.L. (2011). The clinical use of indocyanine green as a near-infrared fluorescent contrast agent for image-guided oncologic surgery. J Surg Oncol.
11 Manizate F., Hiotis S.P., Labow D., Roayaie S., Schwartz M. (2010). Liver functional reserve estimation: state of the art and relevance for local treatments: the Western perspective. J Hepatobiliary Pancreat Sci.
12 Mahounga, D.M., L. Shan, C. Jie, C. Du, S. Wan, and Y. Gu, Synthesis of a Novel L: -Methyl-Methionine-ICG-Der-02 Fluorescent Probe for In Vivo Near Infrared Imaging of Tumors. Mol Imaging Biol, 2012